# [^125^I]Anti-prostate stem cell antigen antibody

Chemical name: | [^125^I]Anti-prostate stem cell antigen antibody
Abbreviated name: | [^125^I]Anti-PSCA antibody
Synonym:
Agent Category: | Antibody
Target: | Prostate stem cell antigen
Target Category: | Antibody-antigen binding
Method of detection: | SPECT, Planar gamma
Source of signal: | ^125^I
Activation: | Not required
Studies: | - Rodents | Click here for Protein (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=protein&id=2909844) and Nucleotide (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=nuccore&id=92141720#feature_92141720) sequence of human PSCA.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=radiolabeled+anti-claudin+4)]

The prostate stem cell antigen (PSCA) is a glycosyl phosphoinositol–anchored cell surface protein that belongs to the Thy-1/Ly-6 class of surface antigens. This protein is so named because it has a 30% homology to the stem cell antigen. Gene expression analysis has shown that PSCA is upregulated in a majority of the human pancreatic cancers and can be used for the classification of cytologically atypical specimens (1, 2). It is also overexpressed in prostate cancer (3), so the use of this antigen as a prostate and pancreatic cancer marker was suggested (3, 4). Although the exact function of the PSCA in pancreatic cancer is unknown, PSCA is an ideal candidate for the development of reagents that can be used for the immunoscintigraphic detection (6) or immunotherapeutic treatment (4) of pancreatic cancer because it has an increased expression specificity for pancreatic adenocarcinoma (1, 5) and has a cell surface location. The development of a pancreatic cancer marker could also help with patient diagnosis or screening of individuals suspected to have a pancreatic cancer. Development of the marker would also assist in the timely detection and treatment of primary or metastatic lesions in individuals and perhaps help prevent further spread of the disease.

A purified rabbit anti-PSCA polyclonal antibody (Ab) (3) was labeled with radioactive iodine (^125^I) and evaluated by in vitro and in vivo investigations (6) for the detection of PSCA expression in pancreatic cancer cell xenografts in mice with severe combined immune deficiency (SCID (http://jaxmice.jax.org/library/notes/453a.html)).

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=labeled+anti-PSCA+antibody+synthsis)]

Generation of the rabbit polyclonal antiserum against PSCA is described by Reiter et al. (3). Briefly, the Ab against a synthetic peptide with a sequence of TARIRAVGLLTVISK was generated in rabbits. For use in the various investigations, the Ab was affinity-purified by using a PSCA-glutathione S-transferase fusion protein.

To label the purified polyclonal Ab with radioactive ^125^I, 20 µg of the Ab in phosphate-buffered saline (PBS; pH 7.5) was dispensed into an iodogen-coated vial and 74–185 MBq (2–5 mCi) ^125^I-labeled sodium iodide in 0.1 M sodium hydroxide (pH 10.0) was added to it. The solution was mixed and allowed to sit at room temperature for 10 min. At the end of incubation, the labeling solution was loaded onto a desalting column to remove any unincorporated ^125^I.

For use as a negative control, a commercially available mAb (http://www.novusbio.com/data_sheet/index/NB110-7722&prev_module=search) against human CD20 was also labeled with ^125^I following the procedure given above.

The radiochemical yield was reported to be between 30–40% and the radiochemical purity as determined by instant thin-layer chromatography (ITLC) was ≥95%. The investigators did not provide the radiofrequency value of the labeled Ab after ITLC. The specific activities of the labeled Abs varied from 0.74–1.295 MBq/6.6 pmol (20–35 µCi/6.6 pmol) of the Ab. The labeled Abs were stored in PBS at 4°C until required and were used within 24 h of labeling.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=labeled+anti-PSCA+antibodies+in+vitro+studies)]

No publications are currently available.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=labeled+anti-PSCA+antibody+rodentia)]

The biodistribution of the ^125^I-labeled anti-PSCA Ab was studied in SCID mice bearing Colo357 xenograft tumors (originating from a human pancreatic adenocarcinoma) (6). SCID mice bearing the Colo357 xenografts were injected with the same amount of either the [^125^I]anti-PSCA or the [^125^I]anti-CD20 mAb. The mice were euthanized at 2, 4, and 6 days after injection and the liver, kidneys, small intestine, bladder, muscle, heart, lungs, stomach, large intestine, spleen, and the tumor were removed and weighed to measure the incorporated radioactivity. Among these tissues, the highest radioactivity uptake values were in the liver, the Colo357 tumors, and the spleen 2 days after administration of the label. Some uptake was also observed in the kidneys. As determined by the tumor/muscle ratio, uptake of the label by the tumors peaked 6 days after the injection. Radioactivity in the liver was suggested to be a result of the enterohepatic metabolism of the labeled Ab and uptake by the spleen indicated Ab sequestration in that organ. The kidney showed an accumulation of the label probably because the Ab metabolites were excreted through the urinary system. By comparison, the labeled CD20 Ab was detected during the same period of time primarily in the spleen because white blood cells have CD20 on the surface and are stored in this organ. Some radioactivity from the labeled CD20 Ab was also detected in the liver, but it exhibited low nonspecific accumulation in the tumors.

For planar gamma single-photon emission computed tomography (SPECT) studies, SCID mice bearing Colo357 cell xenograft tumors (originating from a pancreatic carcinoma) were used. Groups of mice were injected either with the [^125^I]anti-PSCA or the [^125^I]anti-CD20 mAb and the animals were subjected to scintigraphy after 2, 4, and 6 days. Mice injected with the [^125^I]anti-PSCA Ab showed uptake of the radioactivity primarily in the tumors up to 6 days after injection. An uptake of label was also observed in the liver and thyroid during this time. The uptake appeared to be almost equally intense in the liver and the tumors after 6 days. Accumulation of radioactivity in the thyroid was attributed to the dehalogenase activity and the release of ^125^I from the anti-PSCA Ab. During the same period, animals injected with the [^125^I]anti-CD20 Ab showed accumulation of radioactivity primarily in the spleen and liver (because of Ab metabolism in this organ).

SPECT-computed tomography (CT) studies were performed in another group of SCID mice bearing L3.6PL cell pancreatic cancer xenografts (a highly metastatic and aggressive subclone of Colo357 cells). The animals were treated with the [^125^I]anti-PSCA Ab and scintigraphy was performed on the animals after 120 h. The tumor and spleen were clearly visible in these animals despite the location of the tumor within the pancreas. The mice were subsequently euthanized and necropsy was performed to determine the amount of radioactivity present in the liver, spleen, and tumor. Measurement of the radioactivity in these organs revealed that the tumor had almost a 2.5-fold higher label uptake compared to the spleen and an approximately two-fold higher label uptake compared to the liver. No blocking studies that used unlabeled anti-PSCA Ab were performed by the investigators.

The investigators suggested that, although the ^125^I-labeled anti-PSCA Ab appears to be suitable for SPECT-CT to detect pancreatic cancer, this label was suitable only for imaging small animals with the use of a sensitive gamma camera because of its low-energy gamma photon emission. In the clinic the investigators recommend the use of ^123^I-labeled (for SPECT) or ^124^I-labeled (for positron emission tomography) Abs for the detection of PSCA-positive tumors in patients.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=labeled+anti-PSCA+antibody+non-primate+mammals)]

No publications are currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=labeled+anti-PSCA+antibody+non-human+primates)]

No publications are currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=labeled+anti-PSCA+antibody+human+studies)]

No publications are currently available.

## References

1 Argani P., Rosty C., Reiter R.E., Wilentz R.E., Murugesan S.R., Leach S.D., Ryu B., Skinner H.G., Goggins M., Jaffee E.M., Yeo C.J., Cameron J.L., Kern S.E., Hruban R.H. (2001). Discovery of new markers of cancer through serial analysis of gene expression: prostate stem cell antigen is overexpressed in pancreatic adenocarcinoma. Cancer Res.
2 McCarthy D.M., Maitra A., Argani P., Rader A.E., Faigel D.O., Van Heek N.T., Hruban R.H., Wilentz R.E. (2003). Novel markers of pancreatic adenocarcinoma in fine-needle aspiration: mesothelin and prostate stem cell antigen labeling increases accuracy in cytologically borderline cases. Appl Immunohistochem Mol Morphol.
3 Reiter R.E., Gu Z., Watabe T., Thomas G., Szigeti K., Davis E., Wahl M., Nisitani S., Yamashiro J., Le Beau M.M., Loda M., Witte O.N. (1998). Prostate stem cell antigen: a cell surface marker overexpressed in prostate cancer. Proc Natl Acad Sci U S A.
4 Wente M.N., Jain A., Kono E., Berberat P.O., Giese T., Reber H.A., Friess H., Buchler M.W., Reiter R.E., Hines O.J. (2005). Prostate stem cell antigen is a putative target for immunotherapy in pancreatic cancer. Pancreas.
5 Gu Z., Thomas G., Yamashiro J., Shintaku I.P., Dorey F., Raitano A., Witte O.N., Said J.W., Loda M., Reiter R.E. (2000). Prostate stem cell antigen (PSCA) expression increases with high gleason score, advanced stage and bone metastasis in prostate cancer. Oncogene.
6 Foss C.A., Fox J.J., Feldmann G., Maitra A., Iacobuzio-Donohue C., Kern S.E., Hruban R., Pomper M.G. (2007). Radiolabeled anti-claudin 4 and anti-prostate stem cell antigen: initial imaging in experimental models of pancreatic cancer. Mol Imaging.
7 Zervos E.E., Rosemurgy A.S., Al-Saif O., Durkin A.J. (2004). Surgical management of early-stage pancreatic cancer. Cancer Control.